# ^111^In-Labeled lexatumumab

Chemical name: | ^111^In-Labeled lexatumumab
Abbreviated name: | ^111^In-EC-HGS-ETR2
Synonym:
Agent Category: | Antibody
Target: | Tumor necrosis factor–related apoptosis-inducing ligand receptor 2 (TRAILR2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the nucleotice, protein and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=8743&log$=databasead&logdbfrom=protein#refseq) information regarding TRAIL receptors.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1)]

Although anti-growth factor antibodies (Abs) are available for the treatment of cancers (1-3), another technique under investigation to treat this disease is the use of tumor necrosis factor–related apoptosis-inducing ligand (TRAIL) receptor (TRAIL-R) agonist Abs such as mapatumumab and lexatumumab (4, 5). These antibodies (Abs) activate a complex apoptotic pathway in the tumor cell, thereby inducing cell death. The apoptotic pathway and the four TRAIL-R types in humans (designated 1 through 4) have been described in detail by Johnstone et al. (4) and Ashkenazi (5). Lexatumumab (TRM-2 or HGS-ETR2) is a TRAIL-R2 monoclonal antibody (mAb) that targets TRAIL-R2; it is under commercial development and has been approved for clinical trials (http://clinicaltrials.gov/ct2/results?term=lexatumumab) by the United States Food and Drug Administration (USFDA) to treat various cancers. A similar mAb, mapatumumab (TRM-1 or HGS-ETR1), is a TRAIL-R2 mAb that acts as an agonist specifically for the TRAIL-R2 and has been approved by the USFDA for clinical trials (http://clinicaltrials.gov/ct2/results?term=Mapatumumab).

Paclitaxel and docetaxel are anti-cancer drugs that inhibit the mitosis and proliferation of cells by interfering with the depolymerization of microtubules. The mechanism of action of these drugs was discussed in detail by Saloustros et al. (6). Gong et al. observed that the anti-tumor activity of HGS-ETR1 could be enhanced in mice bearing colorectal cancer cell xenograft tumors with pretreatment with paclitaxel (7). Using HGS-ETR2 labeled with radioactive indium (^111^In) (^111^In -EC-HGS-ETR2), the investigators determined that the activity of HGS-ETR2 was increased because the pretreatment with paclitaxel upregulated the expression of TRAIL-R2 in Colo205 cell xenograft tumors in nude mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of ^111^In-EC-HGS-ETR2 was described by Gong et al. (7). Briefly, ethylenedicysteine (EC) was coupled to HGS-ETR2 for the chelation of ^111^In using sulfo-N-hydroxysuccinimide (NHS) and 1-ethyl-3-(3-dimethylaminopropyl)carbodiimide hydrochloride (EDC) as the coupling agents. To do this, EC, NHS, and EDC were mixed with HGS-ETR2 and incubated for 17 h at room temperature. The product, EC-HGS-ETR2, was dialyzed (buffer not described) to remove any unbound reagents. The number of EC per HGS-ETR2, the purification and the yield of EC-HGS-ETR1 was not reported by the investigators. Labeling of EC-HGS-ETR2, to obtain ^111^In-EC-HGS-ETR2, was done performed by adding [^111^In]-indium chloride to a solution of EC-mAb. The purification and yield of the radiolabeled product were not reported. Although the radiochemical purity of ^111^In-EC-HGS-ETR2 was reported to be >95% (determined with radio thin-layer chromatography), the specific activity of the labeled mAb was not reported.

For use as controls during scintigraphic imaging, ^111^In-EC-bovine serum albumin (BSA) and ^111^In-EC-isotype control mAb were also generated as described above (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+in+vitro)]

The steady state levels of TRAIL-R1 and TRAIL-R2 were determined in Colo205 (a human colorectal cancer tumor cell line) and PA-1 (a human ovarian cancer cell line) cells using immunoblots and fluorescence-activated cell sorting (FACS) (7). Both receptor types were expressed in the two cell lines as determined with the immunoblots, but the levels were reported to be higher in the Colo205 cells than in the PA-1 cells. Similar results were obtained with FACS analysis of the two cell lines.

The concentration for 50% inhibition of cell proliferation (IC_50_) for Colo205 cells was determined to be 800 ng/mL and 150 ng/mL for HGS-ETR1 and HGS-ETR2, respectively (7). The PA-1 cells were reported to be resistant to inhibition by both the Abs even at a concentration of 800 ng/mL. This indicated that the number of TRAIL-R1 and -R2 on the PA-1 cell surface was too low to initiate apoptosis on binding of the two respective agonist TRAIL-R mAbs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+rodentia)]

Gong et al. studied the tumor uptake of ^111^In-EC-HGS-ETR2 was studied in nude mice bearing Colo205 xenograft tumors (7). Imaging studies were performed 12 days after inoculation with the cells when the tumor diameter was ~1 cm. The animals (4 or 5 mice/group) were intravenously (IV) injected with either ^111^In-EC-HGS-ETR2, ^111^In-EC-BSA, or the ^111^In-EC-isotype control mAb, and scintigraphic images were obtained 2, 24, and 48 h later. Using computer-outlined regions of interest, the counts per pixel of the tumor site and the normal muscle were used to obtain the tumor/muscle count density ratios (TM ratio). At 2 h after administration of the radiochemicals, little difference in the TM ratios was noted between the controls and the ^111^In-EC-HGS-ETR2–treated animals. However, at 24 and 48 h after the injection of radioactivity, the TM ratios for the ^111^In-EC-HGS-ETR2 and the labeled control-injected animals were reported to be ~3.5–4.5 and ~2, respectively.

In another study, the Colo205 cell xenograft tumor–bearing animals (n = 3 mice) were imaged before and after (at 2 and 24 h after an IV injection of ^111^In-EC-HGS-ETR2) treatment with paclitaxel (7). Animals treated with paclitaxel were imaged 24 h after administration of the drug. When imaging was performed at 2 h after treatment with the labeled mAb, little difference in the TM ratio (~2) was noted in the tumors with or without the paclitaxel treatment. By 24 h the TM ratio was reported to have increased to ~4.2 in tumors of mice treated with paclitaxel compared with a TM ratio of ~2 in the untreated mice. In the same study, PA-1 cell xenograft tumors in animals (n = 3 mice) showed little change in the TM ratio (~1.5) both at 2 and 24 h after the ^111^In-EC-HGS-ETR2 injection. This indicated that very little of the labeled mAb bound to the tumors derived from the PA-1 cells. No blocking studies were reported and the difference in the TM ratios appeared to be stastically small.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Chase J.L. (2008). Clinical use of anti-vascular endothelial growth factor monoclonal antibodies in metastatic colorectal cancer. Pharmacotherapy.
2 Patel D.K. (2008). Clinical use of anti-epidermal growth factor receptor monoclonal antibodies in metastatic colorectal cancer. Pharmacotherapy.
3 Sachdev D., Singh R., Fujita-Yamaguchi Y., Yee D. (2006). Down-regulation of insulin receptor by antibodies against the type I insulin-like growth factor receptor: implications for anti-insulin-like growth factor therapy in breast cancer. Cancer Res.
4 Johnstone R.W., Frew A.J., Smyth M.J. (2008). The TRAIL apoptotic pathway in cancer onset, progression and therapy. Nat Rev Cancer.
5 Ashkenazi A. (2008). Directing cancer cells to self-destruct with pro-apoptotic receptor agonists. Nat Rev Drug Discov.
6 Saloustros E., Mavroudis D., Georgoulias V. (2008). Paclitaxel and docetaxel in the treatment of breast cancer. Expert Opin Pharmacother.
7 Gong J., Yang D., Kohanim S., Humphreys R., Broemeling L., Kurzrock R. (2006). Novel in vivo imaging shows up-regulation of death receptors by paclitaxel and correlates with enhanced antitumor effects of receptor agonist antibodies. Mol Cancer Ther.